# ^111^In-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-MEDI-522

Chemical name: | ^111^In-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-MEDI-522
Abbreviated name: | ^111^In-DOTA-MEDI-522
Synonym: | ^111^In-DOTA-Abegrin, ^111^In-DOTA-Vitaxin
Agent category: | Antibody
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MEDI-522)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). In addition to RGD peptides, a humanized anti-human integrin α_v_β_3_ monoclonal antibody (MEDI-522) was identified to be unique in that it recognizes either the human α_v_ or β_3_ subunit. MEDI-522 cross-reacts with integrin α_v_β_3_ from rabbits, chickens, and hamsters but not with integrin α_v_β_3_ from mice or rats (13). MEDI-522 is being evaluated as an antiangiogenic agent for cancer therapy (14-16). Cai et al. (17) reported the development of ^64^Cu-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-MEDI-522 (^64^Cu-DOTA-MEDI-522) for positron emission tomography imaging of α_v_β_3_ receptors in nude mice bearing tumors. Liu et al. (18) reported the evaluation of ^111^In-DOTA-MEDI-522 for single-photon emission computed tomography (SPECT) imaging α_v_β_3_ receptors in nude mice bearing tumors.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD), MEDI-522 (http://www.clinicaltrials.gov/ct2/results?term=MEDI-522))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20MEDI-522+synthesis)]

DOTA was incubated with EDC and SNHS for 30 min at pH 5.5 with a molar ratio of 10:5:4 (18). The product, DOTA-N-hydroxysulfosuccinimidyl (DOTA-OSSu), was added to MEDI-522 in a molar ratio of 200:1 (DOTA-OSSu/MEDI-522). The reaction mixture was adjusted to pH 8.5 and incubated for ~18 h at 4°C. DOTA-MEDI-522 was purified with column chromatography. DOTA-MEDI-522 (0.33 nmol) was incubated with 74 MBq (2 mCi) ^111^InCl_3_ in sodium acetate buffer (pH 5.5) for 1 h at 39°C. ^111^In-DOTA-MEDI-522 was purified with column chromatography. There were ~10 DOTA moieties per ^111^In-DOTA-MEDI-522. The immunoreactivity was determined to be >90% with integrin α_v_β_3_-positive U87MG human glioblastoma cells. The radiolabeling yield and specific activity of ^111^In-DOTA-MEDI-522 were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20MEDI-522%20in+vitro)]

Liu et al. (18) performed saturation binding studies of ^125^I-MEDI-522 on U87MG cells. ^125^I-MEDI-522 showed a K_d_ value (affinity constant) of 0.35 ± 0.06 nM and a B_max_ value (receptor density) of 2.5 × 10^5^ sites per cell. MEDI-522 and DOTA-MEDI-522 exhibited an inhibition curve similar to that of ^125^I-MEDI-522 binding to U87MG cells. Little binding of ^125^I-MEDI-522 was observed in HT-29 human colon tumor cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20MEDI-522+rodentia)]

Liu et al. (18) performed ex vivo biodistribution studies of 0.74 MBq (0.2 mCi) ^111^In-DOTA-MEDI-522 in nude mice (n = 4/group) bearing human U87MG tumors at 4, 24, 72, 120, and 168 h after injection. Tumor accumulation was 6.19 ± 1.16% injected dose/gram (ID/g), 14.12 ± 0.44% ID/g, 14.85 ± 4.73% ID/g, 11.47 ± 3.51% ID/g, and 11.40 ± 0.07% ID/g at 4, 24, 72, 120, and 168 h after injection, respectively. Radioactivity levels in the blood were 31.3% ID/g and 1.17% ID/g at 4 h and 168 h, respectively. Accumulation in the liver and spleen was 20% ID/g and 16% ID/g at 24 h after injection, respectively. The other normal organs showed less accumulation than the tumor. Co-injection of excess MEDI-522 inhibited tumor accumulation by ~50% at 24 h after injection (P < 0.01). Little inhibition was observed in other normal organs (heart, liver, kidney, and spleen).

SPECT imaging scans were performed in nude mice (n = 3) bearing both U87MG human glioblastoma tumors (high integrin α_v_β_3_ expression) and HT-29 human colon adenocarcinoma tumors (low integrin α_v_β_3_ expression) after injection of 11.1 MBq (0.3 mCi) ^111^In-DOTA-MEDI-522. Radioactivity accumulation was mainly visualized in the heart and abdomen at 2 h after injection. At 24 h, both tumors were gradually visualized. Accumulation of radioactivity was higher in the U87MG tumors than in the HT-29 tumors at 120 h after injection as the radioactivity was cleared from the normal organs. Immunofluorescence staining of tumor sections confirmed binding of MEDI-522 to U87MG tumor cells and not to HT-29 tumor cells. There was no co-localization of MEDI-522 to tumor vasculature in mice with U87MG tumors because MEDI-522 does not cross-react with mouse integrin α_v_β_3_. Anti-mouse β_3_ antibody binding was observed only in mouse tumor vasculature.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20MEDI-522+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20MEDI-522+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20MEDI-522+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Wu H., Beuerlein G., Nie Y., Smith H., Lee B.A., Hensler M., Huse W.D., Watkins J.D. (1998). Stepwise in vitro affinity maturation of Vitaxin, an alphav beta3-specific humanized mAb. Proc Natl Acad Sci U S A.
14 McNeel D.G., Eickhoff J., Lee F.T., King D.M., Alberti D., Thomas J.P., Friedl A., Kolesar J., Marnocha R., Volkman J., Zhang J., Hammershaimb L., Zwiebel J.A., Wilding G. (2005). Phase I trial of a monoclonal antibody specific for alphavbeta3 integrin (MEDI-522) in patients with advanced malignancies, including an assessment of effect on tumor perfusion. Clin Cancer Res.
15 Posey J.A., Khazaeli M.B., DelGrosso A., Saleh M.N., Lin C.Y., Huse W., LoBuglio A.F. (2001). A pilot trial of Vitaxin, a humanized anti-vitronectin receptor (anti alpha v beta 3) antibody in patients with metastatic cancer. Cancer Biother Radiopharm.
16 Gutheil J.C., Campbell T.N., Pierce P.R., Watkins J.D., Huse W.D., Bodkin D.J., Cheresh D.A. (2000). Targeted antiangiogenic therapy for cancer using Vitaxin: a humanized monoclonal antibody to the integrin alphavbeta3. Clin Cancer Res.
17 Cai W., Wu Y., Chen K., Cao Q., Tice D.A., Chen X. (2006). In vitro and in vivo characterization of 64Cu-labeled Abegrin, a humanized monoclonal antibody against integrin alpha v beta 3. Cancer Res.
18 Liu Z., Jia B., Zhao H., Chen X., Wang F. (2011). Specific targeting of human integrin alpha(v)beta (3) with (111)In-labeled Abegrin in nude mouse models. Mol Imaging Biol.